# ^99m^Tc-Labeled acetylated dendrimer poly(amido)-amine generation 5-folic acid-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine pentaacetic acid conjugate

Chemical name: | ^99m^Tc-Labeled acetylated dendrimer poly(amido)-amine generation 5-folic acid-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine pentaacetic acid conjugate
Abbreviated name: | ^99m^Tc-G5-Ac-FA-DTPA
Synonym: | ^99m^Tc-Ac-G5-FA-1B4M DTPA
Agent Category: | Compounds
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=folate+and+dendrimer+and+imaging)]

^99m^Tc-Labeled acetylated (Ac) dendrimer poly(amido)-amine (PAMAM) generation 5 (G5)-folic acid (FA)-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine pentaacetic acid (1B4M DTPA) conjugate, abbreviated as ^99m^Tc-G5-Ac-FA-DTPA, was synthesized by Zhang et al. for folate receptor (FR)-targeted imaging of FR-positive tumors (1, 2).

Folate is an essential vitamin for cell synthesis of nucleotide bases. Some unique features of the FR-folate system make it extremely valuable for developing FR-targeted imaging and therapeutic agents (3-5). First, FR has a high affinity for the exogenous folate conjugates (K_d_ = ~100 pM), but they are inaccessible for the conjugates in most normal tissues. Second, FR-α isoform is overexpressed on ~40% of human cancers, where it is completely accessible to folate conjugates. Third, folate conjugates are taken up by cancer cells via FR-mediated endocytosis, and FR recycles actively to the cell surface with a frequency of 5.7–20 h depending on cell types. Fourth, conjugation of imaging labels via the γ-carboxyl group of folate has no apparent effects on the ligand-binding affinity to FR. Furthermore, folate is a small molecule (MW = ~441) that exhibits rapid and complete penetration of solid tumors and rapid clearance from FR-negative tissues (t_1/2_, <10 min). One disadvantage of the FR-folate system is that FR expresses at a relatively low density on some tumor cell surface (1–3 million FR/cell), which means that the FR-folate binding can be saturated rapidly and the imaging contrast will be limited (3, 4, 6). Sensitive imaging techniques such as positron emission tomography and single-photon emission computed tomography (SPECT) are more desirable for FR-targeted imaging (3, 4, 7). To date, a large set of folate-based radiopharmaceutical agents have been synthesized for nuclear imaging (8). In general, a chelating agent is necessary to bridge the radiolabels and the folate molecule. The chelating agent is also critical for optimizing the molecular properties of conjugates (1, 2, 9).

Dendrimers represent a unique class of nanostructures that are synthesized from branched monomers in a step-wise manner. The molecular properties of dendrimers can be precisely controlled by choosing different branching monomers and surface functional groups (1, 2, 9). PAMAM is one of the most extensively studied dendrimers. Zhang et al. synthesized two folate-based compounds, ^99m^Tc-G5-Ac-pegFA-DTPA and ^99m^Tc-G5-Ac-FA-DTPA, and one control, ^99m^Tc-G5-Ac-DTPA, with PAMAM G5 dendrimer and folate (1, 2). To increase the solubility and decrease the nonspecific cellular uptake of the agents, the primary amines on the surface of PAMAM dendrimers were partially converted to acetamide moieties, which were used to link with the bifunctional chelating agent 1B4M DTPA. Folate was either PEGylated or left unPEGylated, and its c-carboxyl group was used to conjugate with the primary amine of PAMAM. The two folate-based conjugates exhibited excellent stability, rapid clearance from blood, and high accumulation in tumor xenografts (1, 2). This chapter describes the results obtained with ^99m^Tc-G5-Ac-FA-DTPA. Another chapter in MICAD describes the data obtained with ^99m^Tc-G5-Ac-pegFA-DTPA (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- FR-targeted chapters (http://www.ncbi.nlm.nih.gov/books/?term=folate%20receptor%20AND%20micad%5bbook%5d) on MICAD
- Protein (http://www.ncbi.nlm.nih.gov/protein/?term=Folate+Receptor) and nucleotide (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Folate+Receptor) information of FR
- FR-targeted clinical trials (http://clinicaltrials.gov/ct2/results?term=Folate+Receptor) in Clinicaltrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20350006)]

Zhang et al. described the synthesis of ^99m^Tc-G5-Ac-pegFA-DTPA, ^99m^Tc-G5-Ac-FA-DTPA, and ^99m^Tc-G5-Ac-DTPA (1, 2). The primary amines on the surface of G5 PAMAM dendrimers were first partially converted to acetamide moieties (G5-Ac, yield = 94.7%). PEGylated folate (NHS-PEG1540-FA) was synthesized through reactions of N-hydroxysuccinimide ester of FA with poly(ethylene glycol)bis amine (NH_2_-PEG1540-NH_2_). Conjugation of the folate or PEGylated folate to the dendrimers was achieved via condensation between the γ-carboxyl group of folate and the primary amine of dendrimer (G5-Ac-FA or G5-Ac-pegFA, yield = 90.8%). The partially acetylated dendrimers were then linked with the chelating agent 1B4M DTPA to generate G5-Ac-FA-DTPA, G5-Ac-pegFA-DTPA, or G5-Ac-DTPA (yield = 98.2%). Each G5-Ac-DTPA contained 77 acetyl and 8 DTPA molecules. Each G5-Ac-FA-DTPA contained 77 acetyl, 4.8 folic acid molecules, and 7 DTPA molecules, and each G5-Ac-pegFA-DTPA contained 77 acetyl, 5.2 folic acid molecules, and 8 DTPA molecules. Therefore, the three compounds (G5-Ac-pegFA-DTPA, G5-Ac-FA-DTPA, and G5-Ac-DTPA) contained a similar number of DTPA molecules (i.e., 7 or 8 molecules). The two folate conjugates (G5-Ac-pegFA-DTPA and G5-Ac-FA-DTPA) contained a similar number of folic acid molecules (i.e., 4.8 to 5.2 molecules).

Radiolabeling was performed after reduction of ^99m^TcO4− to reduced ^99m^Tc using stannous chloride. The radiochemical yield and radioactivity of the three radiolabeled agents were >95% and 88.3 ± 1.0%, respectively. They were used for experiments without further purification. The partition ratios (log P) between n-octanol and water were −2.030, −2.061, and −2.167 for ^99m^Tc-G5-Ac-FA-DTPA, ^99m^Tc-G5-Ac-pegFA-DTPA, and ^99m^Tc-G5-Ac-DTPA, respectively, indicating that the agents had high water solubility.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20350006)]

The in vitro stability was analyzed after incubation of the ^99m^Tc-G5-Ac-FA-DTPA, ^99m^Tc-G5-Ac-pegFA-DTPA, and ^99m^Tc-G5-Ac-DTPA with phosphate-buffered saline and new-born calf serum, respectively. After incubation for 6 h at 37ºC, at least 86% and 84% of the agents kept their original structure in phosphate-buffered saline and in new-born calf serum, respectively, indicating high stability.

Cell uptake of the three agents was quantitatively measured with FR-expressing KB cells (a human oral epidermoid carcinoma line) (1, 2). In vitro cell binding of the ^99m^Tc-G5-Ac-pegFA-DTPA was ~15% of total added radioactivity after incubation for 6 h at 37ºC, whereas ^99m^Tc-G5-Ac-FA-DTPA and the control ^99m^Tc-G5-Ac-DTPA exhibited lower binding ability (~11% and ~10%, respectively).

These results indicated that conjugation of FA directly to PAMAM dendrimers did not improve the cell uptake. In contrast, conjugation through a PEG spacer could improve the cellular internalization. Uptake of the three agents in the KB cells grown in FA-rich medium (to inhibit FR expression) was similar (<10%), suggesting no significant binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20350006)]

The in vivo studies on stability after injection into mice (n = 3/time point) showed that 80.45% of the ^99m^Tc-G5-Ac-FA-DTPA, and 80.56% of the ^99m^Tc-G5-Ac-DTPA remained intact within 6 h in blood of normal mice (1, 2).

The pharmacokinetics of the agents was studied in normal mice (n = 5). A rapid decrease was observed at 30 min after injection, followed by a slow clearance. The plasma half-life was estimated to be 13.75 min for the ^99m^Tc-G5-Ac-FA-DTPA and 12.73 min for the control ^99m^Tc-G5-Ac-DTPA. Less than 10% of the injected agents remained in circulation after 6 h (assuming that blood represents 5.5% of the total body mass).

Biodistribution was investigated with KB tumor–bearing nude mice (n = 3/time point). The mice were maintained on a folate-deficient diet for the duration of experiment to minimize the circulating levels of FA. Both ^99m^Tc-G5-Ac-DTPA and ^99m^Tc-G5-Ac-FA-DTPA were cleared rapidly from the blood, decreasing from 11.75% injected dose/gram (ID/g) at 2 h to 5.60% ID/g at 6 h for ^99m^Tc-G5-Ac-DTPA and from 12.59% ID/g at 2 h to 4.00% ID/g at 6 h for ^99m^Tc-G5-Ac-FA-DTPA. Both agents remained at a low level up to 6 h in the FR-negative organs, including brain.

The kidneys, which express FR, are the major clearance organs. The level of nontargeted ^99m^Tc-G5-Ac-DTPA decreased from 32.08% ID/g at 2 h to 26.06% ID/g at 6 h. In contrast, the level of ^99m^Tc-G5-Ac-FA-DTPA increased slightly with time (22.06% ID/g at 2 h to 28.18% ID/g at 6 h). In the liver, the concentrations of nontargeted ^99m^Tc-G5-Ac-DTPA decreased with clearance from blood (41.07% ID/g at 2 h to 32.94% ID/g at 6 h), whereas the targeted ^99m^Tc-G5-Ac-FA-DTPA decreased more slowly (32.02% ID/g at 2 h to 26.17% ID/g at 6 h). In the tumors, the level of ^99m^Tc-G5-Ac-FA-DTPA increased from 3.10% ID/g at 2 h to 6.78% ID/g at 6 h. The nontargeted ^99m^Tc-G5-Ac-DTPA also increased slightly from 2.81% ID/g at 2 h to 4.38% ID/g at 6 h.

Micro-SPECT imaging confirmed the predominant uptake of ^99m^Tc-G5-Ac-FA-DTPA in the FR-positive tumors, liver, and kidneys in the KB tumor–bearing mice (n = 2/time point) (1, 2). Comparison among ^99m^Tc-G5-Ac-pegFA-DTPA, ^99m^Tc-G5-Ac-FA-DTPA, and ^99m^Tc-G5-Ac-DTPA showed that PEGylation of the PAMAM dendrimer-FA conjugate improves the tumor targeting and may be used as a targeted delivery system for imaging labels and therapeutic drugs (1, 2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Zhang Y., Sun Y., Xu X., Zhu H., Huang L., Zhang X., Qi Y., Shen Y.M. (2010). Radiosynthesis and micro-SPECT imaging of 99mTc-dendrimer poly(amido)-amine folic acid conjugate. Bioorg Med Chem Lett.
2 Zhang Y., Sun Y., Xu X., Zhang X., Zhu H., Huang L., Qi Y., Shen Y.M. (2010). Synthesis, biodistribution, and microsingle photon emission computed tomography (SPECT) imaging study of technetium-99m labeled PEGylated dendrimer poly(amidoamine) (PAMAM)-folic acid conjugates. J Med Chem.
3 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
4 Low P.S., Kularatne S.A. (2009). Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
5 Zhao X., Li H., Lee R.J. (2008). Targeted drug delivery via folate receptors. Expert Opin Drug Deliv.
6 Miotti S., Bagnoli M., Ottone F., Tomassetti A., Colnaghi M.I., Canevari S. (1997). Simultaneous activity of two different mechanisms of folate transport in ovarian carcinoma cell lines. J Cell Biochem.
7 Altiparmak B., Lambrecht F.Y., Bayrak E., Durkan K. (2010). Design and synthesis of 99mTc-citro-folate for use as a tumor-targeted radiopharmaceutical. Int J Pharm.
8 Low P.S., Henne W.A., Doorneweerd D.D. (2008). Discovery and development of folic-acid-based receptor targeting for imaging and therapy of cancer and inflammatory diseases. Acc Chem Res.
9 Konda S.D., Aref M., Wang S., Brechbiel M., Wiener E.C. (2001). Specific targeting of folate-dendrimer MRI contrast agents to the high affinity folate receptor expressed in ovarian tumor xenografts. MAGMA.